# [^18^F]Norchloro-fluoro-homoepibatidine

Chemical name: | [^18^F]Norchloro-fluoro-homoepibatidine
Abbreviated name: | [^18^F]NCFHEB
Synonym:
Agent Category: | Compound
Target: | Neuronal α4β2 nicotinic acetylcholine receptor (nAChR)
Target Category: | Receptor-ligand binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Other Non-primate Mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NCFHEB)]

Neuronal α4β2 nicotinic cholinergic receptors (nAChRs) are part of a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine causes a rapid increase in cellular permeability to ions, such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α receptors (α2 to α10) and four subtypes of structural β receptors (β2 to β5). nAChRs have been found to be involved in cognitive processes such as learning memory and control of movement in normal subjects. nAChR dysfunction has been implicated in a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease, and Parkinson's disease. nAChRs also play a significant role in nicotine addiction and other health problems associated with tobacco smoking.

3-[2(S)-2-Azetidinylmethoxy]pyridine (A-85380) is a highly potent and selective α4β2 nAChR agonist with subnanomolar affinity (4, 5). 6-[^18^F]Fluoro-A-85380 and 2-[^18^F]fluoro-A-85380 have been studied in humans as positron emission tomography (PET) agents for α4β2 nAChR imaging in the brain. A-85380 has also been labeled as 5-[^123^I]iodo-3-[2(S)-2-azetidinylmethoxy]pyridine (5-[^123^I]iodo-A-85380 (5-[^123^I]IA)), which has been developed as a single-photon emission computed tomography (SPECT) agent for the non-invasive study of nAChR in the brain. However, prolonged imaging times (2–4 h) are required for reliable quantification because of the slow kinetics of this agent. Norchloro-fluoro-homoepibatidine (NCFHEB), an analog of epibatidine, is a highly potent and selective α4β2 nAChR antagonist with subnanomolar affinity (6). NCFHEB has been shown to be a functional antagonist of α4β2 nAChR in mice. [^18^F]NCFHEB is being developed as a PET agent for the noninvasive study of α4β2 nAChR in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NCFHEB%20and%20synthesis)]

Deuther-Conrad et al. (7) reported synthesis of [^18^F]NCFHEB by a two-step procedure, which consisted of standard ([^18^F]KF/Kryptofix 2.2.2) ^18^F-nucleophilic aromatic fluorination of N-ethoxycarbonyl-norchloro-bromo-homoepibatidine and deprotection of the product. Enantiomers ((+)[^18^F]NCFHEB and (-)[^18^F]NCFHEB) were separated with high-performance liquid chromatography. Average radiochemical yield was 2% (end of synthesis, based on [^18^F]KF) for each enantiomer. Time of synthesis, radiochemical purity, and specific activity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NCFHEB%20and%20in%20vitro)]

Deuther-Conrad et al. (6) reported that (+)NCFHEB exhibited inhibition constant (K_i_) values (obtained with the use of [^3^H]epibatidine) of 0.064 ± 0.005, 3.81 ± 0.87, and 31.7 ± 21.7 nM in human α4β2, α3β4, and α7 receptors, respectively. (-)NCFHEB exhibited K_i_ values of 0.112 ± 0.035, 2.58 ± 0.89, and 119 ± 69 nM in human α4β2, α3β4, and α7 receptors, respectively. On the other hand, 2-fluoro-A-85380 exhibited K_i_ values of 0.069 ± 0.028, 86.4 ± 29.6, and 317 (n =1) nM in human α4β2, α3β4, and α7 receptors, respectively. Therefore, NCFHEB enantiomers exhibit binding affinities to these receptors that are similar to the binding affinities of 2-fluoro-A-85380, with a lower K_i,α3β4_/K_i,α4β2_ ratio than 2-fluoro-A-85380. (-)NCFHEB, (+)NCFHEB, and 2-fluoro-A-85380 had K_i_ values of 0.069, 0.512, and 0.475 nM for α4β2 in rat thalamic membranes, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NCFHEB%20and%20rodentia)]

Deuther-Conrad et al. (7) reported biodistribution studies of (+)[^18^F]NCFHEB and (-)[^18^F]NCFHEB in mice, showing peak accumulation in the brain of 7.45% injected dose/gram (ID/g) and 5.60% ID/g at 20 min, respectively. Co-injection or pretreatment of 2-fluoro-A-85380, (-)NCFHEB, or (+)NCFHEB reduced the radioactivity in the brain by 50% to 76%. The urinary bladder had the highest accumulation (~50% ID/g), followed by the kidney (>10% ID/g) and the liver (~10% ID/g). Little radioactivity accumulation was observed in the femur. The total brain accumulation of 2-[^18^F]fluoro-A-85380 was 3.20% ID/g at 20 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NCFHEB%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

Brust et al. (8) used PET imaging to compare the kinetics of the two enantiomers of [^18^F]NCFHEB with 2-[^18^F]fluoro-A85380 in the porcine brain. Juvenile female pigs (n = 24) were studied with PET using [^18^F]NCFHEB; in a parallel experiment, nine animals received an injection (1 mg/kg) of the nAChR agonist A81418 before radiotracer administration followed by infusion (2 mg/kg per 7 h). Several compartment models were performed for quantification. (-)[^18^F]NCFHEB and (+)[^18^F]NCFHEB showed brain accumulation two to three times greater than 2-[^18^F]fluoro-A-85380. All three radiotracers displayed spatially heterogeneous binding kinetics in brain regions with high (thalamus and hippocampus), moderate (striatum and cortex), or low (cerebellum) specific binding. The equilibrium of the specific binding of (-)[^18^F]NCFHEB was reached in ~2 h, which was earlier than that of (+)[^18^F]NCFHEB or 2-[^18^F]fluoro-A85380. Continuous administration of A81418 significantly inhibited the specific binding of (-)[^18^F]NCFHEB and (+)[^18^F]NCFHEB (P < 0.05) by 51% to 72% in the thalamus and hippocampus. Moderate inhibition was observed in the striatum and cortex (24% to 50%) and marginal inhibition (11% to 36%) was observed in the cerebellum. The peripheral metabolism of (-)NCFHEB and (+)[^18^F]NCFHEB proceeded slowly with ~40% to 50% intact at 90 min after injection.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NCFHEB%20and%20(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NCFHEB%20and%20human)]

No publication is currently available.

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Abreo M.A., Lin N.H., Garvey D.S., Gunn D.E., Hettinger A.M., Wasicak J.T., Pavlik P.A., Martin Y.C., Donnelly-roberts D.L., Anderson D.J., Sullivan J.P., Williams M., Arneric S.P., Holladay M.W. (1996). Novel 3-Pyridyl ethers with subnanomolar affinity for central neuronal nicotinic acetylcholine receptors. J Med Chem.
5 Sullivan J.P., Donnelly-Roberts D., Briggs C.A., Anderson D.J., Gopalakrishnan M., Piattoni-Kaplan M., Campbell J.E., McKenna D.G., Molinari E., Hettinger A.M., Garvey D.S., Wasicak J.T., Holladay M.W., Williams M., Arneric S.P. (1996). A-85380 [3-(2(S)-azetidinylmethoxy) pyridine]: in vitro pharmacological properties of a novel, high affinity alpha 4 beta 2 nicotinic acetylcholine receptor ligand. Neuropharmacology.
6 Deuther-Conrad W., Patt J.T., Feuerbach D., Wegner F., Brust P., Steinbach J. (2004). Norchloro-fluoro-homoepibatidine: specificity to neuronal nicotinic acetylcholine receptor subtypes in vitro. Farmaco.
7 Deuther-Conrad W., Patt J.T., Lockman P.R., Allen D.D., Patt M., Schildan A., Ganapathy V., Steinbach J., Sabri O., Brust P. (2008). Norchloro-fluoro-homoepibatidine (NCFHEB) - a promising radioligand for neuroimaging nicotinic acetylcholine receptors with PET. Eur Neuropsychopharmacol.
8 Brust P., Patt J.T., Deuther-Conrad W., Becker G., Patt M., Schildan A., Sorger D., Kendziorra K., Meyer P., Steinbach J., Sabri O. (2008). In vivo measurement of nicotinic acetylcholine receptors with [18F]norchloro-fluoro-homoepibatidine. Synapse.